# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-PEGylated cyclic arginine-glycine-aspartic acid peptide

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-PEGylated cyclic arginine-glycine-aspartic acid peptide
Abbreviated name: | ^64^Cu-DOTA-PEG-c(RGDyK)
Synonym: | ^64^Cu-Pegylated c(RGDyK)
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29)]

^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-PEGylated cyclic arginine-glycine-aspartic acid peptide [^64^Cu-DOTA-PEG-c(RGDyK)] is an integrin-targeted molecular imaging agent developed for positron emission tomography (PET) of tumor vasculature and tumor angiogenesis (1). ^64^Cu is a positron emitter with a physical half-life (t_½_) of 12.8 h.

Cellular survival, invasion, and migration control embryonic development, angiogenesis, tumor metastasis, and other physiological processes (2, 3). Among the molecules that regulate angiogenesis are integrins, which comprise a superfamily of cell adhesion proteins that form heterodimeric receptors for extracellular matrix (ECM) molecules (4, 5). These transmembrane glycoproteins consist of two noncovalently associated subunits, α and β (18 α- and 8 β-subunits in mammals), which are assembled into at least 24 α/β pairs. Several integrins, such as integrin α_v_β_3_, have affinity for the arginine-glycine-aspartic acid (RGD) tripeptide motif, which is found in many ECM proteins. Expression of integrin α_v_β_3_ receptors on endothelial cells is stimulated by angiogenic factors and environments. The integrin α_v_β_3_ receptor is generally not found in normal tissue, but it is strongly expressed in vessels with increased angiogenesis, such as tumor vasculature. It is significantly upregulated in certain types of tumor cells and in almost all tumor vasculature.

Molecular imaging probes that carry the RGD motif that binds to the integrin α_v_β_3_ can be used to image tumor vasculature and evaluate angiogenic responses to tumor therapy (6, 7). Various RGD peptides in both linear and cyclic forms (RGDfK or RGDyK) have been developed for in vivo binding to integrin α_v_β_3_ (8). Chen et al (9). evaluated a cyclic RGD D-Tyr analog peptide [c(RGDyK)] labeled with ^64^Cu or ^18^F in nude mice bearing breast tumor. Chen et al. used 1,4,7,10-tetrazadodecane-N,N',N'',N'''-tetraacetic acid (DOTA) for c(RGDyK) conjugation with ^64^Cu. ^64^Cu-DOTA-c(RGDyK) showed prolonged tumor radioactivity retention but persistent liver radioactivity. To improve the pharmacokinetics and tumor retention of the radiolabeled peptide, Chen et al. (10) modified c(RGDyK) with monofunctional methoxy-polyethylene glycol (PEG; molecular weight = 2,000) and showed that the modified PEGylated RGD peptide had faster blood clearance, lower kidney uptake, and prolonged tumor uptake. Using the same strategy, Chen et al. (1) inserted a heterobifunctional PEG linker (molecular weight = 3,400) between DOTA and c(RGDyK) to produce ^64^Cu-DOTA-PEG-c(RGDyK). The PEG moiety appeared to improve the in vivo kinetics of this PET radioligand.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20synthesis)]

Chen et al. (1) reported the synthesis of ^64^Cu-DOTA-PEG-c(RGDyK). The c(RGDyK) peptide was first prepared via solution cyclization of fully protected linear pentapeptide H-Gly-Asp(OtBu)-D-Tyr(OtBu)-Lys(Boc)-Arg(Pbf)-OH, followed by trifluoroacetic acid (TFA) deprotection in the presence of the free radical scavenger triisopropylsilane. The c(RGDyK)-PEG conjugate was prepared by coupling c(RGDyK) with t-butoxycarbonyl (t-Boc)-protected PEG-succinimidyl ester (t-Boc-NH-PEG-CO_2_Su). The t-Boc protecting group was unblocked by TFA cleavage. DOTA was obtained commercially. The DOTA-PEG-c(RGDyk) conjugate was prepared by in situ activation of DOTA by 1-ethyl-3-[3-(dimethylamino)propyl]carbodiimide (EDC) and N-hydroxysulfonosuccinimide (SNHS) in a molar ratio of 10:5:4 (DOTA:EDC:SNHS).The c(RGDyk)-PEG conjugate in water at 4ºC was added to the resultant DOTA-sulfosuccinimydyl ester (OSSu), and the pH was adjusted to 8.5. The reaction mixture was incubated overnight at 4ºC. The DOTA-PEG-c(RGDyk) conjugate was then purified by semipreparative high-performance liquid chromatography (HPLC). The molecular weight of the DOTA-PEG-c(RGDyK) conjugate was determined to be 4,400 by mass spectrometry, which appeared to agree with the theoretical value. The purified product was labeled with ^64^Cu by addition of ^64^Cu in the ratio of 5–25 μg peptide per 37 MBq (1 mCi) ^64^Cu in 0.1-N sodium acetate buffer (pH 5.5). This was followed by incubation at 50ºC for 45 minutes. The reaction was terminated by addition of ethylenediaminetetraacetic acid (EDTA). ^64^Cu-DOTA-PEG-c(RGDyK) was purified with a C-18 Sep-Pak cartridge that used 85% ethanol as the elution solvent. The radiochemical purities were 50%, 80%, 95%, and ≥98% for 5, 10, 15, and 20 μg peptide, respectively. The specific activity of ^64^Cu-DOTA-PEG-c(RGDyK) ranged from 14,800 to 29,600 GBq/mmol (400 to 800 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20in%20vitro)]

Solid-phase receptor-binding assays of unlabeled DOTA-PEG-c(RGDyK) were conducted by competitive displacement of ^125^I-labeled echistatin binding to purified human α_v_β_3_ integrin (1). The inhibition concentration (IC_50_) was 67.5 ± 10.5 nM. In comparison, the IC_50_ for unpegylated DOTA-c(RGDyK) was 31.2 ± 5.8 nM. In a hydrophilicity study, the octanol-water partition coefficient (LogP_OCT_) for ^64^Cu-DOTA-PEG-c(RGDyK) was determined to be −2.97 ± 0.30 (n = 3). The LogP_OCT_ for ^64^Cu-DOTA-c(RGDyK) was −2.8 ± 0.04.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20rodentia)]

Biodistribution studies of ^64^Cu-DOTA-PEG-c(RGDyK) were conducted in nude mice bearing s.c. U87MG glioblastomas (0.4–0.6 cm in diameter) (1). Each mouse received 370 kBq (10 μCi) of ^64^Cu-DOTA-PEG-c(RGDyK) by i.v. administration. The radioligand was rapidly cleared from the blood and most organs, and the kidneys appeared to be the primary route of excretion. The radioactivity levels (n = 4) in the tumor were 2.74 ± 0.45% injected dose/g (% ID/g) and 1.62 ± 0.18% ID/g at 0.5 h and 4 h, respectively. The blood radioactivity levels were 0.57 ± 0.15% ID/g and 0.02 ± 0.02% ID/g at 0.5 h and 2 h, respectively. The kidney radioactivity level was ~3.2% ID/g (extrapolated from Figure 3) at 0.5 h and decreased to ~1.2% ID/g at 4 h. The liver activity was 0.58 ± 0.07% ID/g at 4 h. Overall, the authors suggested that PEGylation had a minimal effect on tumor uptake and clearance. When compared to the unPEGylated radioligand, the PEGylated radioligand also had a relatively faster renal clearance and a lower liver accumulation. Coinjection of 10 mg/kg unlabeled c(RGDyK) peptide decreased the radioactivity of ^64^Cu-DOTA-PEG-c(RGDyK) in all tissues except the kidneys. The radioactivity level of the tumor at 1 h was reduced from 2.21 ± 0.38% ID/g to 0.22 ± 0.03% ID/g.

Imaging of 14.8 MBq (400 μCi) ^64^Cu-DOTA-PEG-c(RGDyK) with microPET at 1 h in nude mice bearing the U87MG tumor clearly visualized the tumor with high contrast relative to the contralateral background (1). The kidneys, intestinal tract, and urinary bladder were also visible on the image. Digital whole-body autoradiography of the mice after PET imaging showed a distribution pattern similar to of the patterns observed in the biodistribution and imaging studies. The radioactivity levels in the tumor, liver, and kidneys were 2.6 ± 0.6% ID/g, 0.8 ± 0.2% ID/g, and 2.4 ± 0.5% ID/g, respectively. In a single mouse, PET imaging also visualized a U87MG tumor implanted into the mouse forebrain with a tumor/brain ratio of 4.0 ± 0.5. However, the absolute tumor radioactivity level was only 0.4 ± 0.1% ID/g.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20%29%20AND%20human)]

No publication is currently available.

## References

1 Chen X., Hou Y., Tohme M., Park R., Khankaldyyan V., Gonzales-Gomez I., Bading J.R., Laug W.E., Conti P.S. (2004). Pegylated Arg-Gly-Asp peptide: 64Cu labeling and PET imaging of brain tumor alphavbeta3-integrin expression. J Nucl Med.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Paulhe F., Manenti S., Ysebaert L., Betous R., Sultan P., Racaud-Sultan C. (2005). Integrin function and signaling as pharmacological targets in cardiovascular diseases and in cancer. Curr Pharm Des.
4 Hood J.D., Cheresh D.A. (2002). Role of integrins in cell invasion and migration. Nat Rev Cancer.
5 Hwang R., Varner J. (2004). The role of integrins in tumor angiogenesis. Hematol Oncol Clin North Am.
6 Cai W., Shin D.W., Chen K., Gheysens O., Cao Q., Wang S.X., Gambhir S.S., Chen X. (2006). Peptide-labeled near-infrared quantum dots for imaging tumor vasculature in living subjects. Nano Lett.
7 Massoud T.F., Gambhir S.S. (2003). Molecular imaging in living subjects: seeing fundamental biological processes in a new light. Genes Dev.
8 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
9 Chen X., Park R., Tohme M., Shahinian A.H., Bading J.R., Conti P.S. (2004). MicroPET and autoradiographic imaging of breast cancer alpha v-integrin expression using 18F- and 64Cu-labeled RGD peptide. Bioconjug Chem.
10 Chen X., Park R., Shahinian A.H., Bading J.R., Conti P.S. (2004). Pharmacokinetics and tumor retention of 125I-labeled RGD peptide are improved by PEGylation. Nucl Med Biol.